# Ligand-conjugated, gold-doped CdHgTe quantum dots for multispectral imaging

Chemical name: | Ligand-conjugated gold-doped CdHgTe quantum dots for multispectral imaging
Abbreviated name: | QD800-RGD, QD820-anti-CEACAM1, and QD840-anti-EGFR
Synonym:
Agent Category: | Nanoparticles
Target: | Integrin αvβ3, carcinoembryonic antigen-related cell adhesion molecule 1 (CEACAM1), and epidermal growth factor receptor (EGFR)
Target Category: | Receptors
Method of detection: | Optical imaging
Source of signal / contrast: | Quantum dots (QDs)
Activation: | No
Studies: | - In vitro; - Rodents | No structure available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=multispectral%20imaging%20and%20quantum%20dots)]

Three ligand-conjugated, gold-doped CdHgTe (Au:CdHgTe) quantum dots (QDs), abbreviated as QD800-RGD, QD820-anti-CEACAM1, and QD840-anti-EGFR, respectively, were synthesized by Han et al. for multispectral imaging (MSI) of multiple biomarkers in tumors (1).

MSI is a technique that enables acquisition of spectrally resolved information at each pixel of an imaged scene. It solves some of the challenges in fluorescence-based imaging, e.g., eliminating tissue autofluorescence (2). In living subjects, MSI provides an effective means to quantify multiple biomarkers simultaneously (3, 4). To this end, QDs have been considered to be an attractive molecule label for use with MSI in the past decade because of their high fluorescence efficiency, minimal photobleaching, and constant excitation wavelengths together with sharp and symmetrical tunable emission spectra (5). QDs are spherical semiconductor nanocrystals, which are composed of elements from periodic groups of II–VI (CdSe) or III–V (InP) (5). They are typically synthesized by injection of liquid precursors into hot organic solvents, which enables generation of nanocrystals with different sizes by altering the amount of precursors and crystal growth time. The quantum yield reported in the literature ranges from less than 10% to up to 80%, depending on the materials, synthetic methods, and physicochemical properties of QDs (1, 6).

Han et al. synthesized an array of near-infrared (NIR) Au:CdHgTe QDs by doping gold into the CdHgTe QDs, which enhances the photoluminescence and reduces the cytotoxicity (1). The Au:CdHgTe QDs were monodispersed with tunable NIR fluorescence (740–840 nm). The quantum yield (QY) of Au:CdHgTe QDs reached 48%, which was higher than that of undoped CdHgTe QDs (42%) and Au nanoclusters (<2%) (1). To detect multiple tumor biomarkers simultaneously with MSI, these QDs were conjugated with three different ligands: RGD peptide targeting integrin α_v_β_3_, and monoclonal antibodies targeting carcinoembryonic antigen-related cell adhesion molecule 1 (CEACAM1) and epidermal growth factor receptor (EGFR) (1). This chapter summarizes the data obtained with the three Au:CdHgTe QD conjugate mixtures.

### Related Resource Links:

Nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/?term=integrin%20alpha%20v%20beta%203) and protein (http://www.ncbi.nlm.nih.gov/protein?term=integrin%20alpha%20v%20beta%203) information of integrin α_v_β_3_

Nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=carcinoembryonic%20antigen-related%20cell%20adhesion%20molecule%201) and protein (http://www.ncbi.nlm.nih.gov/protein?term=carcinoembryonic%20antigen-related%20cell%20adhesion%20molecule%201) information of CEACAM1

Nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=epidermal%20growth%20factor%20receptor) and protein (http://www.ncbi.nlm.nih.gov/protein?term=epidermal%20growth%20factor%20receptor) information of EGFR

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22447216)]

Han et al. detailed the synthesis of the three Au:CdHgTe QD conjugates (1). Gold was first doped into the CdHgTe QDs by refluxing a mixed solution of CdCl_2_, HgCl_2_, AuCl_3_, and KHTe for 5–60 min at 96°C under a slow N_2_ flow in the presence of L-cysteine and L-glutathione as stabilizers. The Au dopant concentration (6.2% relative to the Cd molar concentration) was confirmed with inductively coupled plasma mass spectrometry. The emission peak shifted from 740 to 840 nm with prolonged refluxing time. The QY of as-prepared Au:CdHgTe QDs was 48% relative to that of 1,1'-dioctadecyltetramethyl indotricarbocyanine iodide (28%) under identical absorbance illumination conditions (0.037 a.u. at 747 nm).

The photostability of Au:CdHgTe QDs in water determined with spectrofluorometry was slightly higher than that of undoped CdHgTe QDs (1). After continuous optical excitation (λ_ex_, 640 nm; λ_em_, 840 nm) for 120 sec, the Au:CdHgTe QDs preserved 90.7% of their fluorescence, and the undoped CdHgTe QDs preserved 87.9%. Under transmission electron microscopy, the Au:CdHgTe QDs were uniform and monodispersed with an average diameter of 6–8 nm. The X-ray diffraction analysis of the powder Au:CdHgTe indicated that they had a cubic zinc blende structure, similar to the CdHgTe_2_ (ICDD PDF 65-6126).

The RGD peptide and antibodies against CEACAM1 and EGFR were linked to Au:CdHgTe QD800, QD820, and QD840, respectively, with N-hydroxysuccinimide and 1-ethyl-3-(3-dimethylaminopropyl)carbodiimide as cross-linkers. The QD/antibody and QD/RGD molar ratios were ~1:6 and ~1:160, respectively, in the conjugation reaction. The conjugation time was 1 h at room temperature. The excess quenching reagent and free RGD peptides were removed with ultrafiltration, and the QD-antibody conjugates were separated from free antibodies with gel filtration. The QD conjugates were verified with agarose gel electrophoresis. The conjugation efficiencies for RGD peptides and antibodies were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22447216)]

The in vitro cytotoxicity of Au:CdHgTe QDs was evaluated with A549 lung cancer cells after incubation with varied concentrations of QDs for 24 h (1). The half-maximal inhibitory concentration (IC_50_) of the Au:CdHgTe QDs was measured to be 158.63 μg/mL (95% confidence limits: 142.79–182.60 μg/mL), whereas this value for the CdHgTe QDs was 84.17 μg/mL (95% confidence limits: 66.91–106.27 μg/mL). The A549 cells maintained >80% viability after treatment for 48 h with Au:CdHgTe QDs at concentrations as high as 100 μg/mL. In contrast, the viability of A549 cells treated with CdHgTe QDs at concentrations of 20–160 μg/mL decreased dramatically, suggesting that Au:CdHgTe QDs had a lower cytotoxicity than undoped CdHgTe QDs. Reduced cytotoxicity of the Au:CdHgTe QDs was considered to be due to the doping with Au and capping with glutathione and cysteine because the surface chemistry of QDs plays an important role in cytotoxicity in addition to the components of QDs themselves.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22447216)]

The toxicity of QDs to mice was determined after tail vein injection of six doses (16, 20, 26, 32, 40, and 50 mg/kg body mass, respectively) of Au:CdHgTe QDs or CdHgTe to ICR mice (n = 5 males and 5 females/group) (1). The lethal dose (LD) measurement showed that the LD_5_, LD_50_, and LD_95_ of the Au:CdHgTe QDs were 25.35, 34.92, and 48.11 mg/kg, respectively. The 95% confidence limits for LD_50_ of the Au:CdHgTe QDs were 31.37–39 mg/kg. The LD_5_, LD_50_, and LD_95_ for CdHgTe QDs were 19.11, 29.93, and 46.88 mg/kg, respectively, with 95% confidence limits of 26.34–33.98 mg/kg for LD_50_. These results demonstrated that Au:CdHgTe QDs was less toxic to mice than CdHgTe QDs.

In vivo MSI was performed at 2 h after tail vein injection of the three QD conjugate mixture (~25 nM for each conjugate) to A549 tumor xenograft-bearing mice (1). In the mouse given QD conjugate mixture, the fluorescence signal was observed in the primary tumor, metastatic lesion, and lymphatic basin. The signals from QD800-RGD, QD820-anti-CEACAM1, and QD840-anti-EGFR were co-localized with certain differences in their distribution. Semi-quantification of the signal intensity (counts/sec) showed an order of lymphatic basin (0.41) > primary tumor (0.35) > metastatic lesion (0.17) for QD800-RGD; lymphatic basin (0.27) > metastatic lesion (0.16) > primary tumor (0.07) for QD820-anti-CEACAM1; and lymphatic basin (0.35) > metastatic lesion (0.25) > primary tumor (0.22) for QD840-anti-EGFR. The signal in the primary tumor from QD820-anti-CEACAM1 was much lower than that from QD800-RGD and QD840-anti-EGFR, which might be due to the expression difference of the three targets. These results indicated that the Au:CdHgTe QD conjugates could be used as probes for in vivo detection of multiple tumor markers simultaneously. The control mouse and mouse given unconjugated QDs showed no fluorescence signal in tumors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term)]

No references are currently available.

## References

1 Han S., Mu Y., Zhu Q., Gao Y., Li Z., Jin Q., Jin W. (2012). Au:CdHgTe quantum dots for in vivo tumor-targeted multispectral fluorescence imaging. Anal Bioanal Chem.
2 Byers R.J., Hitchman E.R. (2011). Quantum dots brighten biological imaging. Prog Histochem Cytochem.
3 Cassette, E., Helle, M., Bezdetnaya, L., Marchal, F., Dubertret, B., and Pons, T. Design of new quantum dot materials for deep tissue infrared imaging. Adv Drug Deliv Rev. 2012
4 Zhou L., El-Deiry W.S. (2009). Multispectral fluorescence imaging. J Nucl Med.
5 Tholouli E., Sweeney E., Barrow E., Clay V., Hoyland J.A., Byers R.J. (2008). Quantum dots light up pathology. J Pathol.
6 Li J., Wu D., Miao Z., Zhang Y. (2010). Preparation of quantum dot bioconjugates and their applications in bio-imaging. Curr Pharm Biotechnol.